# 3-N-(2-[^18^F]Fluoroethyl)spiperone

Chemical name: | 3-N-(2-[^18^F]Fluoroethyl)spiperone
Abbreviated name: | [^18^F]FESP
Synonym:
Agent Category: | Compound
Target: | D_2_ dopamine receptor and 5-HT_2_ serotonin receptor
Target Category: | Receptor
Method of detection: | PET
Source of signal / contrast: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents; - Non-human primates; - Humans | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%223-N-%282-fluoroethyl%29spiperone%22%5BSubstance%20Name%5D)]

Dopamine, a neurotransmitter, plays an important role in the mediation of movement, cognition, and emotion (1, 2). Dopamine shortage plays a role in various neuropsychiatric disorders, such as Parkinson’s disease (PD), schizophrenia, autism, attention deficit hyperactivity disorder, and drug abuse. Two subtypes of dopamine receptors, D_1_ and D_2_, were well-characterized pharmacologically and biochemically (3). D_2_ dopamine receptors have been implicated in the pathophysiology of PD, Alzheimer's disease, and schizophrenia (4).

Serotonin (5-hydroxytryptamine, 5-HT) has diverse physiological roles as a neurotransmitter in the central nervous system (5). It also is a regulator of smooth muscle function and platelet aggregation. The brain cortical 5-HT system has been implicated in several neuropsychiatric disorders, including major depression, anxiety, obsessive-compulsive disorder, and schizophrenia (6, 7).

Spiperone and its analog, 3-N-(2-fluoroethyl)spiperone (FESP) are high-affinity D_2_ dopamine and 5-HT_2_ serotonin receptor antagonists, showing a low affinity for α1-adrenergic receptors and marginal binding to other receptors (8). 3-N-(2-[^18^F]Fluoroethyl)spiperone ([^18^F]FESP) has been studied as a positron emission tomography (PET) tracer for imaging D_2_ and 5HT_2_ receptor densities. It has also used as a reporter probe for dopamine D_2_ receptor in imaging transgene expression in rodents (9-11).

### Related Resource Links:

- Chapters in MICAD (5-HT_2A_ (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=5-HT2A+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad), Dopamine receptors (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=dopamine%20(receptors%20OR%20receptor)+%20AND+Table+AND+micad%5Bbook%5D))
- Gene information in NCBI (5-HT_2A_ (http://www.ncbi.nlm.nih.gov/gene/3356), D_2_ receptor, (http://www.ncbi.nlm.nih.gov/gene/1813) D_3_ receptor (http://www.ncbi.nlm.nih.gov/gene/1814))
- Articles in Online Mendelian Inheritance in Man (OMIM) (5-HT_2A_ (http://www.ncbi.nlm.nih.gov/omim/182135), D_2_ receptor (http://www.ncbi.nlm.nih.gov/omim/126450), D_3_ receptor (http://www.ncbi.nlm.nih.gov/omim/126451))
- Clinical trials (5-HT_2A_ (http://www.clinicaltrials.gov/ct2/results?term=5-HT2A), Dopamine receptors (http://www.clinicaltrials.gov/ct2/results?term=dopamine+receptor))
- Drug information in Food and Drug Administration (5-HT_2A_ (http://google2.fda.gov/search?q=5-HT2a&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=8&y=1), Dopamine receptors (http://google2.fda.gov/search?q=dopamine+receptor&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=6&y=12))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%223-N-%282-fluoroethyl%29spiperone%22%5BSubstance%20Name%5D%20AND%20synthesis%5BAll%20Fields%5D)]

[^18^F]FESP can be synthesized by either N-alkylation or nucleophilic substitution (12-15). Alkylation of the amide nitrogen in spiperone by [^18^F]fluorobromoethane in the presence of NaOH provided [^18^F]FESP in 35-40% radiochemical yield (5-8% overall radiochemical yield). [^18^F]Fluorobromoethane was easily prepared by the reaction of 1,2-bromoethane with potassium [^18^F]fluoride Kryptofix complex in 15-20% radiochemical yield. The radiochemical purity of [^18^F]FESP was found to be >99% by high-performance liquid chromatography (HPLC). The specific activity was 185-370 GBq/μmol (5-10 Ci/μmol) at the end of synthesis with a total synthesis time of 70 min.

A one-step, one-pot synthesis of [^18^F]FESP using nucleophilic fluorination of 3-(2'-bromoethyl)spiperone or 3-(2'-methylsulfonyloxyethyl)spiperone with K[^18^F]F/Kryptofix2.2.2 in acetonitrite in <60 min was performed (12). This method provided a 99% chemical purity and a specific activity of 74-370 GBq/μmol (2-10 Ci/μmol) at the end of synthesis (EOS). The radiochemical yield was 30-40% (EOS).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%223-N-%282-fluoroethyl%29spiperone%22%5BSubstance%20Name%5D%20AND%20in%20vitro)]

FESP was reported to have selective binding affinity to D_2_ (striatum) and 5-HT_2_ (frontal cortex) receptor sites in homogenates of rat brain membranes (8). The K_i_ values for D_2_ and 5-HT_2_ were 0.44 nM and 0.57 nM, respectively. It has a K_i_ value of 23 nM for the α1-adrenergic receptor in rat forebrain membrane and negligible binding to other sites.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%223-N-%282-fluoroethyl%29spiperone%22%5BSubstance%20Name%5D%20AND%20rodentia)]

Biodistribution studies in rats showed a high uptake of radioactivity in the lung (1.80% injected dose (ID)/g), kidney (1.00% ID/g), spleen (0.97% ID/g), and liver (0.82% ID/g) at 15 min after injection of [^18^F]FESP (16). The brain had a low uptake of 0.18% ID/g. Low radioactivity was observed in bone tissue, indicating little defluorination. [^18^F]FESP remained 90% intact in the brain striatum, 32% in the cerebellum, and 46% in the frontal cortex for up to 4 h after injection. In mice, [^18^F]FESP remained 90% intact in the brain striatum, and 62% in the cerebellum for up to 3.5 h after injection (17). [^18^F]FESP was metabolized peripherally with only 11% intact [^18^F]FESP in rat plasma at 2 h after injection (16).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%223-N-%282-fluoroethyl%29spiperone%22%5BSubstance%20Name%5D%20AND%20%28dog%20or%20pig%20or%20rabbit%20or%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%223-N-%282-fluoroethyl%29spiperone%22%5BSubstance%20Name%5D%20AND%20primate%20not%20human)]

[^18^F]FESP PET studies in non-human primates have provided useful assessment of the D_2_ and 5-HT_2_ receptor in the brain (16-21). Coenen et al. (18) showed a selective uptake in striatum (0.048% ID/cm^3^) over the frontal cortex (0.0088% ID/cm^3^) and in the cerebellum (0.0056% ID/cm^3^) in baboon brains at 4 h after injection. The striatum D_2_ receptor sites in the striatum were saturable. The striatum [^18^F]FESP uptake was blocked by pretreatment with excess unlabeled FESP (0.5 mg/kg) and (+)-butaclamol (0.5 mg/kg), a D_1_/D_2_ antagonist (22). Ritanserin and ketanserin, 5-HT_2_ antagonists, had no effect on [^18^F]FESP uptake in the striatum and blocked only 15-20% [^18^F]FESP uptake in the frontal cortex. [^18^F]FESP arterial plasma activity rapidly decreased to 25% at 1 h and 8% at 4 h after injection. D_2_ receptor density (B_max_) was estimated by two PET studies to be 25.9 ± 12.7 pmol/g (19) and 37.5 ± 11.5 pmol/g (21). Using serial PET scans, 5-HT_2_ receptor density was estimated to be 35.6 ± 10.9 pmol/g in the baboon frontal cortex (20).

## Human Studies

[[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%223-N-%282-fluoroethyl%29spiperone%22%5BSubstance%20Name%5D%20AND%20humans)]

Human dosimetry was estimated based on human dynamic PET scans after injection of 37 MBq (1 mCi) [^18^F]FESP (23). The gallbladder received the highest dose (0.207 mGy/MBq or 797 mrad/mCi). Other organs that received high doses were the urinary bladder (0.083 mGy/MBq or 308 mrad/mCi) and liver (0.065 mGy/MBq or 110 mrad/mCi). The total body dose was 0.0119 mGy/MBq (44 mrad/mCi).

[^18^F]FESP PET studies of D_2_ receptor distribution in human brain were reported, showing a localization of radioactivity in the striatum (16, 24, 25). Only about 1% of [^18^F]PESP entered the brain. [^18^F]FESP was metabolized peripherally with 54% intact [^18^F]FESP in arterial plasma at 2 h after injection (16). Striatal-to-cerebellum ratio and kinetic constants are commonly used as analytical parameters in [^18^F]FESP PET studies. Wienhard et al. (25) reported on [^18^F]FESP PET studies in 30 patients with various disorders related to the dopaminergic system and in 6 normal subjects. PET brain scans of normal subjects showed that the highest uptake was in the caudate and pituitary, followed by the cortex and cerebellum at 3 h after injection of 185 MBq (5 mCi) [^18^F]FESP. PET scans of patients showed decreases in the number of available D_2_ receptors in the striatum and striatum-to-cerebellum ratio. Patients with brain damage also showed both low [^18^F]FDG and [^18^F]FESP uptake in the striatum.

5-HT_2_ receptor distribution in human brain were studied by [^18^F]FESP PET in 20 healthy volunteers and 34 patients with unipolar depression (26) There was a significant reduction of binding capacity in 19 non-drug-treated patients as compared with healthy controls in the cortical regions but not in the striatum. In paroxetine-treated patients (n = 15), there was no significant difference between the drug-treated patients and healthy volunteers. Paroxetine is a specific serotonin reuptake inhibitor. Paroxetine treatment led to remission in these patients. Chronic treatment with fluvoxamine (27), another specific serotonin reuptake inhibitor, significantly increased the in vivo binding of [^18^F]FESP in the frontal and occipital cortex but not in the striatum of drug-naïve, unipolar, depressed patients (n = 9).

[^18^F]FESP PET is useful for objective monitoring of D_2_ and 5-HT_2_ receptor sites in patients with serotonergic and dopaminergic disorders. It revealed stage-related changes in depression and dopaminergic disorders. [^18^F]FESP has also demonstrated its usefulness as a PET tracer in the imaging of non-functioning pituitary adenomas from meningiomas and craniopharyngiomas (28).

## References

1 Carbon M., Ghilardi M.F., Feigin A., Fukuda M., Silvestri G., Mentis M.J., Ghez C., Moeller J.R., Eidelberg D. (2003). Learning networks in health and Parkinson's disease: reproducibility and treatment effects. Hum Brain Mapp.
2 Chesselet M.F., Delfs J.M. (1996). Basal ganglia and movement disorders: an update. Trends Neurosci.
3 Stoof J.C., Kebabian J.W. (1984). Two dopamine receptors: biochemistry, physiology and pharmacology. Life Sci.
4 Seeman P., Bzowej N.H., Guan H.C., Bergeron C., Reynolds G.P., Bird E.D., Riederer P., Jellinger K., Tourtellotte W.W. (1987). Human brain D1 and D2 dopamine receptors in schizophrenia, Alzheimer's, Parkinson's, and Huntington's diseases. Neuropsychopharmacology.
5 Lucki I. (1998). The spectrum of behaviors influenced by serotonin. Biol Psychiatry.
6 Abi-Dargham A., Laruelle M., Aghajanian G.K., Charney D., Krystal J. (1997). The role of serotonin in the pathophysiology and treatment of schizophrenia. J Neuropsychiatry Clin Neurosci.
7 Charney D.S. (1998). Monoamine dysfunction and the pathophysiology and treatment of depression. J Clin Psychiatry.
8 Goffinet A.M., Leysen J., Labar D. (1990). In vitro pharmacological profile of 3-N-(2-fluoroethyl)spiperone. J Cereb Blood Flow Metab.
9 MacLaren D.C., Gambhir S.S., Satyamurthy N., Barrio J.R., Sharfstein S., Toyokuni T., Wu L., Berk A.J., Cherry S.R., Phelps M.E., Herschman H.R. (1999). Repetitive, non-invasive imaging of the dopamine D2 receptor as a reporter gene in living animals. Gene Ther.
10 Yaghoubi S.S., Wu L., Liang Q., Toyokuni T., Barrio J.R., Namavari M., Satyamurthy N., Phelps M.E., Herschman H.R., Gambhir S.S. (2001). Direct correlation between positron emission tomographic images of two reporter genes delivered by two distinct adenoviral vectors. Gene Ther.
11 Chen I.Y., Wu J.C., Min J.J., Sundaresan G., Lewis X., Liang Q., Herschman H.R., Gambhir S.S. (2004). Micro-positron emission tomography imaging of cardiac gene expression in rats using bicistronic adenoviral vector-mediated gene delivery. Circulation.
12 Satyamurthy N., Bida G.T., Barrio J.R., Luxen A., Mazziotta J.C., Huang S.C., Phelps M.E. (1986). No-carrier-added 3-(2'-[18F]fluoroethyl)spiperone, a new dopamine receptor-binding tracer for positron emission tomography. Int J Rad Appl Instrum B.
13 Satyamurthy N., Barrio J.R., Bida G.T., Huang S.C., Mazziotta J.C., Phelps M.E. (1990). 3-(2'-[18F]fluoroethyl)spiperone, a potent dopamine antagonist: synthesis, structural analysis and in-vivo utilization in humans. Int J Rad Appl Instrum [A].
14 Chi D.Y., Kilbourn M.R., Katzenellenbogen J.A., Brodack J.W., Welch M.J. (1986). Synthesis of no-carrier-added N-([18F]fluoroalkyl)spiperone derivatives. Int J Rad Appl Instrum [A].
15 Kiesewetter D.O., Eckelman W.C., Cohen R.M., Finn R.D., Larson S.M. (1986). Syntheses and D2 receptor affinities of derivatives of spiperone containing aliphatic halogens. Int J Rad Appl Instrum [A].
16 Barrio J.R., Satyamurthy N., Huang S.C., Keen R.E., Nissenson C.H., Hoffman J.M., Ackermann R.F., Bahn M.M., Mazziotta J.C., Phelps M.E. (1989). 3-(2'-[18F]fluoroethyl)spiperone: in vivo biochemical and kinetic characterization in rodents, nonhuman primates, and humans. J Cereb Blood Flow Metab.
17 Coenen H.H., Laufer P., Stocklin G., Wienhard K., Pawlik G., Bocher-Schwarz H.G., Heiss W.D. (1987). 3-N-(2-[18F]-fluoroethyl)-spiperone: a novel ligand for cerebral dopamine receptor studies with pet. Life Sci.
18 Coenen H.H., Wienhard K., Stocklin G., Laufer P., Hebold I., Pawlik G., Heiss W.D. (1988). PET measurement of D2 and S2 receptor binding of 3-N-[(2'-18F]fluoroethyl)spiperone in baboon brain. Eur J Nucl Med.
19 Huang S.C., Bahn M.M., Barrio J.R., Hoffman J.M., Satyamurthy N., Hawkins R.A., Mazziotta J.C., Phelps M.E. (1989). A double-injection technique for in vivo measurement of dopamine D2-receptor density in monkeys with 3-(2'-[18F]fluoroethyl)spiperone and dynamic positron emission tomography. J Cereb Blood Flow Metab.
20 Jovkar S., Wienhard K., Coenen H.H., Pawlik G., Heiss W.D. (1991). Quantification of baboon cortical S2 serotonin receptors in vivo with 3-N-(2'-F18)fluoroethylspiperone and positron emission tomography. Eur J Nucl Med.
21 Jovkar S., Wienhard K., Pawlik G., Coenen H.H. (1990). The quantitative analysis of D2-dopamine receptors in baboon striatum in vivo with 3-N-[2'-18F]fluoroethylspiperone using positron emission tomography. J Cereb Blood Flow Metab.
22 Schetz J.A., Kim O.J., Sibley D.R. (2003). Pharmacological characterization of mammalian D1 and D2 dopamine receptors expressed in Drosophila Schneider-2 cells. J Recept Signal Transduct Res.
23 Herzog H., Coenen H.H., Kuwert T., Langen K.J., Feinendegen L.E. (1990). Quantification of the whole-body distribution of PET radiopharmaceuticals, applied to 3-N-([18F]fluoroethyl)spiperone. Eur J Nucl Med.
24 Bahn M.M., Huang S.C., Hawkins R.A., Satyamurthy N., Hoffman J.M., Barrio J.R., Mazziotta J.C., Phelps M.E. (1989). Models for in vivo kinetic interactions of dopamine D2-neuroreceptors and 3-(2'-[18F]fluoroethyl)spiperone examined with positron emission tomography. J Cereb Blood Flow Metab.
25 Wienhard K., Coenen H.H., Pawlik G., Rudolf J., Laufer P., Jovkar S., Stocklin G., Heiss W.D. (1990). PET studies of dopamine receptor distribution using [18F]fluoroethylspiperone: findings in disorders related to the dopaminergic system. J Neural Transm Gen Sect.
26 Messa C., Colombo C., Moresco R.M., Gobbo C., Galli L., Lucignani G., Gilardi M.C., Rizzo G., Smeraldi E., Zanardi R., Artigas F., Fazio F. (2003). 5-HT(2A) receptor binding is reduced in drug-naive and unchanged in SSRI-responder depressed patients compared to healthy controls: a PET study. Psychopharmacology (Berl).
27 Moresco R.M., Colombo C., Fazio F., Bonfanti A., Lucignani G., Messa C., Gobbo C., Galli L., Del Sole A., Lucca A., Smeraldi E. (2000). Effects of fluvoxamine treatment on the in vivo binding of [F-18]FESP in drug naive depressed patients: a PET study. Neuroimage.
28 Lucignani G., Losa M., Moresco R.M., Del Sole A., Matarrese M., Bettinardi V., Mortini P., Giovanelli M., Fazio F. (1997). Differentiation of clinically non-functioning pituitary adenomas from meningiomas and craniopharyngiomas by positron emission tomography with [18F]fluoro-ethyl-spiperone. Eur J Nucl Med.